# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-HB22.7

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-HB22.7
Abbreviated name: | ^64^Cu-DOTA-HB22.7
Synonym:
Agent category: | Antibody
Target: | CD22
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4126455) and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=933) for more information about the CD22.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HB22.7)]

CD22 is a transmembrane glycoprotein found on B lymphocytes. It functions as an adhesion molecule binding to sialic acid–bearing ligands with an immunoglobulin (Ig) domain and also modulates signal transduction via the B-cell receptor (1). CD22 is expressed on the cell surface of mature B cells and non-Hodgkin’s lymphomas (2). HB22.7, an anti-CD22 monoclonal antibody (mAb), blocks the interaction of the Ig domain of CD22 with its ligands to induce proliferation in primary B cells and apoptosis in neoplastic B cells (3, 4). 1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) has been successfully coupled to HB22.7 and labeled with ^64^Cu to produce a potential molecular imaging agent to target non-Hodgkin’s lymphomas (5). ^64^Cu is a positron emitter with a physical half-life of 12.7 h and is suitable for positron emission tomography (PET) imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HB22.7+and+synthesis)]

Martin et al. (5) reported the synthesis of ^64^Cu-DOTA-HB22.7. The HB22.7 mAb (67 nM) was incubated with 670 nM DOTA-NHS-ester in 0.1 M tetramethyl ammonium phosphate (pH 8.0) for 2.5 h at 37°C. DOTA-HB22.7 was isolated with column filtration. There were 6.3 DOTA molecules per antibody molecule. A mixture of DOTA-HB22.7 and ^64^Cu in 0.25 M ammonium acetate was incubated at 40°C for 40–60 min. ^64^Cu-DOTA-HB22.7 was purified with column filtration with a radiochemical yield of 83%. The radiochemical purity was >99% with a specific activity of 56 MBq/nmol (1.5 mCi/nmol) at the time of injection.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HB22.7+AND+in+vitro)]

Martin et al. (5) performed flow cytometric analysis with DOTA-HB22.7 and HB22.7 using the CD22-expressing human Raji lymphoma cell line with a fluorescent-labeled anti-IgG as the secondary antibody. Binding of DOTA-HB22.7 and HB22.7 to Raji cells exhibited the same mean fluorescent intensity of 110 units, indicating that the immunoreactivity of DOTA-HB22.7 was similar to the parent mAb.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HB22.7+AND+rodentia)]

Martin et al. (5) performed PET imaging studies in nude mice (n = 3/group) bearing Raji tumor xenografts. Each mouse received 7.4 MBq (0.2 mCi) ^64^Cu-DOTA-HB22.7 by intravenous injection. The radioactivity levels were obtained at 3 h, 24 h, and 48 h after injection, with tumor uptake values in percent injected dose per cc (% ID/cc) of 1.8, 5.5, and 6.8, respectively; tumor retention was high. Intraperitoneal and subcutaneous injections showed similar tumor uptakes at 24 and 48 h. Biodistribution studies at 48 h showed that the tumor (~18% ID/g) and blood (17–24% ID/g) exhibited the highest radioactivity levels for the three routes of injections. The distribution patterns to other nontargeted organs were similar with the exception of the spleen (14% ID/g), which showed the highest uptake with the intraperitoneal route compared with the other two routes (8% ID/g). The liver, kidneys, heart, lungs, and urinary bladder had similar radioactivity levels of ~5% ID/g. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HB22.7+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HB22.7+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HB22.7+AND+human)]

No publication is currently available.

## NIH Support

R24 CA86307, R24 CA110804, R33 CA89706

## References

1 Tedder T.F., Tuscano J., Sato S., Kehrl J.H. (1997). CD22, a B lymphocyte-specific adhesion molecule that regulates antigen receptor signaling. Annu Rev Immunol.
2 Haas K.M., Sen S., Sanford I.G., Miller A.S., Poe J.C., Tedder T.F. (2006). CD22 ligand binding regulates normal and malignant B lymphocyte survival in vivo. J Immunol.
3 Tedder T.F., Poe J.C., Haas K.M. (2005). CD22: A Multifunctional Receptor That Regulates B Lymphocyte Survival and Signal Transduction. Adv Immunol.
4 Tuscano J.M., Riva A., Toscano S.N., Tedder T.F., Kehrl J.H. (1999). CD22 cross-linking generates B-cell antigen receptor-independent signals that activate the JNK/SAPK signaling cascade. Blood.
5 Martin, S.M., R.T. O'Donnell, D.L. Kukis, C.K. Abbey, H. McKnight, J.L. Sutcliffe, and J.M. Tuscano, Imaging and Pharmacokinetics of (64)Cu-DOTA-HB22.7 Administered by Intravenous, Intraperitoneal, or Subcutaneous Injection to Mice Bearing Non-Hodgkin's Lymphoma Xenografts. Mol Imaging Biol, 2008